# 2-chloro-N-((S)-((S)-1-[^11^C]methylpiperidine-2-yl)(thiophen-3-yl)methyl)-3-(trifluoromethyl)benzamide ([^11^C]SA1) and derivatives

Chemical name: | 2-chloro-N-((S)-((S)-1-[^11^C]methylpiperidine-2-yl)(thiophen-3-yl)methyl)-3-(trifluoromethyl)benzamide ([^11^C]SA1) and derivatives | [image]
Abbreviated name: | [^11^C]SA1, [^11^C]SA2, and [^11^C]SA3 | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | Glycine transporter 1 (GlyT-1) | [image]
Target Category: | Amino acid transporter | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^11^C | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents; - Non-human primates | Structures of [^11^C]SA1, [^11^C]SA2 and [^11^C]SA3 (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=glycine%20transporter&cmd=DetailsSearch)]

The amino acid (aa) glycine acts as a neurotransmitter in the mammalian central nervous system (CNS) and modulates the neuroexcitatory activity of the N-methyl-D-aspartate (NMDA) receptor (NMDAR) through strychnine-insensitive glycine binding sites located on the receptor (for details regarding structure and function of NMDAR, see Paoletti et al. (2)). Impaired functioning of the NMDAR is believed to be responsible for the cognitive dysfunction (e.g., loss of reasoning, hallucinations, etc.) observed in individuals suffering from neuropsychiatric ailments, such as schizophrenia and related disorders; improving the activity of this receptor has been shown to be therapeutic (3, 4). Because glycine is an obligatory co-agonist of the NMDAR in the presence of D-serine, the glycine binding site on the receptor is considered to be a suitable therapeutic target for the treatment of schizophrenia (4). Specific sodium chloride-dependent transporters are responsible for transporting glycine into the CNS. However, rapid sequestration into the nerve terminals and surrounding glial cells by two high-affinity transporters, designated as GlyT-1 and GlyT-2, block the activity of glycine on the NMDAR in the synapse (4). GlyT-1 has been shown to maintain low levels of glycine at the synapse, which indicates that the aa participates in controlling the process of neurotransmission through the NMDAR (4). It has been hypothesized that inhibition of GlyT-1 would increase glycine concentrations around the synapse (because by inhibiting the GlyT-1 transporter glycine will not be sequestered into the surrounding glial cells), which would enhance the activity of the NMDAR. The use of GlyT-1 inhibitors could be a good approach to treat schizophrenia and other related cognitive afflictions (5). In addition, researchers are interested in using noninvasive imaging techniques to study any changes in the brains of individuals suffering from neuropsychiatric disorders that may be associated with the GlyT-1. Therefore, several imaging agents, such as [^18^F]2,4-dichloro-N-((1-(propylsulphony)-4-(6-fluoropyridine-2-yl)piperidine-4-yl)methyl)benzamide ([^18^F]MK-6577 (6)) and [^11^C]GSK931145 (7), that can be used with positron emission tomography (PET) were developed and successfully evaluated in non-human primates ([^18^F]MK-6577 and [^11^C]GSK931145) and humans ([^11^C]GSK931145) for the in vivo visualization of GlyT-1. Toyohara et al. reported the development of three new ^11^C-labeled non-sarcosine GlyT-1 inhibitors (2-chloro-N-((S)-((S)-1-[^11^C]methylpiperidine-2-yl)(thiophen-3-yl)methyl)-3-(trifluoromethyl)benzamide ([^11^C]SA1), N-((S)-((S)-1-[^11^C]methylpiperidine-2-yl)(phenyl)methyl)thiophene-2-carboxamide ([^11^C]SA2), and 2-chloro-N-((S)-((S)-1-[^11^C]methylpiperidine-2-yl)(phenyl)methyl)-3-(trifluoromethyl)benzamide ([^11^C]SA3)) and investigated the biodistribution of these tracers in mice (1). Among these radiolabeled compounds, [^11^C]SA1 was evaluated with PET to visualize GlyT-1 in the brain of rhesus monkeys (Macaca mulatta).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=amino+acid+transporter+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Human GlyT-1 variant 3 protein and nucleotide sequences (http://www.genome.jp/dbget-bin/www_bget?refseq:NM_001024845) (RefSeq database)

GlyT-1 in Online Mendelian Inheritance in Man (OMIM) Database (http://omim.org/entry/601019)

GlyT-1 in Kyoto Encyclopedia of Genes and Genomics Database (http://www.genome.jp/dbget-bin/www_bget?hsa:6536)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=GlyT-1) related to GlyT-1

NMDAR in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=nmdar)

What is schizophrenia? (http://www.nimh.nih.gov/health/publications/schizophrenia/what-is-schizophrenia.shtml) (National Institute of Mental Health web site)

Treatment (http://www.nimh.nih.gov/health/publications/schizophrenia/how-is-schizophrenia-treated.shtml) for schizophrenia (National Institute of Mental Health web site)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DSA1%20synthesis&cmd=DetailsSearch)]

The synthesis of SA1, SA2, and SA3 is detailed in international patent applications WO 03/089411 A1 (2003), WO 2005/037781 A2 (2005), and WO 2005/037792 A1 (2005) (1). The labeling of these compounds with ^11^C has been described by Toyohara et al. (1). The radiochemical yields of [^11^C]SA1, [^11^C]SA2, and [^11^C]SA3 were 50 ± 10%, 66 ± 22%, and 56 ± 3%, respectively. The radiochemical purity of each probe was >97%, as determined with high-performance liquid chromatography, and the specific activities of the tracers at 30 min after the end of bombardment (this was the total time taken for the synthesis, purification, and formulation of the labeled compounds) were 20–89 GBq/μmol (0.54–2.4 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DSA1%20in%20vitro&cmd=DetailsSearch)]

The 50% inhibition concentrations of SA1, SA2, and SA3 that inhibited the uptake of [^3^H]gly in mouse synaptosomes were determined to be 9.0 ± 2.0, 6,400 ± 1,930, and 39.7 ± 17.4 nM, respectively (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DSA1%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^11^C]SA1, [^11^C]SA2, and [^11^C]SA3 was studied in normal mice (n = 4 animals/tracer per time point) after an intravenous injection of the labeled compounds (2.0 MBq/0.043–0.078 nmol (54 mCi/0.043–0.078 nmol) (1). The animals were euthanized at various time points ranging from 1 min to 60 min postinjection (p.i.), and the organs of interest were harvested to determine the amount of radioactivity accumulated in the various tissues (presented as percent of injected dose per gram tissue (% ID/g)). The amount of label detected in the different tissues is presented in Table 1.

Table 1: Amount of radioactivity from [ ^ 11 ^ C]SA1, [ ^ 11 ^ C]SA2, and [ ^ 11 ^ C]SA3 present in various tissues of mice.

Tissue | [ ^ 11 ^ C]SA1 | | | [ ^ 11 ^ C]SA2 | | | [ ^ 11 ^ C]SA3
Tissue | Time (min) post injection
Tissue | 5 | 15 | 60 | 5 | 15 | 60 | 5 | 15 | 60
Tissue | % Injected dose/g tissue
Blood* | 0.7 ± 0.1 | 0.4 ± 0.1 | 0.3 ± 0.1 | 0.7 ± 0.1 | 0.6 ± 0.1 | 0.5 ± 0.0 | 0.9 ± 0.1 | 0.7 ± 0.1 | 0.7 ± 0.1
Lung | 29.0 ± 6.5 | 14.0 ± 1.4 | 3.6 ± 0.6 | 19.5 ± 1.7 | 8.0 ± 0.9 | 2.3 ± 0.4 | 24.4 ± 6.5 | 14.2 ± 2.1 | 3.8 ± 0.7
Liver | 7.8 ± 1.0 | 12.5 ± 2.6 | 7.6 ± 1.4 | 4.6 ± 0.5 | 6.2 ± 0.8 | 6.4 ± 1.7 | 4.8 ± 0.5 | 5.1 ± 0.6 | 4.3 ± 0.4
Kidney | 10.8 ± 1.0 | 6.2 ± 0.9 | 1.9 ± 0.4 | 12.8 ± 2.3 | 8.0 ± 0.7 | 3.4 ± 0.5 | 10.6 ± 0.7 | 7.5 ± 1.6 | 2.8 ± 0.6
Brain | 2.1 ± 0.3 | 2.0 ± 0.1 | 0.9 ± 0.1 | 1.0 ± 0.1 | 0.8 ± 0.1 | 0.3 ± 0.1 | 1.6 ± 0.1 | 1.7 ± 0.2 | 0.9 ± 0.1

* Data for other time points (1 min p.i. and 30 min p.i.) and tissues (heart, pancreas, spleen, small intestine, and muscle) is available in Toyohara et al. ( 1 ).

The patterns of uptake of radioactivity from the three probes in the different tissues were similar. In the brain, the uptake peaked at 15 min p.i. and gradually decreased thereafter. The uptake of label in the brain was higher with [^11^C]SA1 than with either [^11^C]SA2 (lowest uptake in brain) or [^11^C]SA3. Time-activity curves for the medulla oblongata, cerebellum, and cortex for the three tracers showed there was a heterogeneous distribution of radioactivity in these regions of the brain, which was consistent with the level of GlyT-1 in these tissues: medulla oblongata > cerebellum > cortex.

In a blocking study, mice were injected with [^11^C]SA1 (2.0 MBq/0.065 nmol (54 mCi/0.065 nmol)) and [^11^C]SA3 (2.0 MBq/0.074 nmol (54 mCi/0.074 nmol)) in the presence of 0.01, 0.1, and 1.0 mg/kg body weight unlabeled SA1 and SA3, respectively (n = 5 animals/concentration of unlabeled SA1 and SA3) (1). The animals were euthanized 15 min or 30 min later for [^11^C]SA1 and [^11^C]SA3, respectively, and the brains were harvested to determine the amount of radioactivity present in different regions of the organ (Table 2). Co-injection of [^11^C]SA1 with unlabeled SA1 deceased uptake of the labeled probe significantly (P < 0.05) in the medulla oblongata and the cerebellum (GlyT-1 rich regions) compared to controls, whereas no such reduction in uptake was apparent with [^11^C]SA3.

Table 2: Uptake of radioactivity in cerebellum and medulla oblongata from [ ^ 11 ^ C]SA1 and [ ^ 11 ^ C]SA3 in presence of different doses of unlabeled SA1 and SA3, respectively.

Probe | Brain tissue* | Control (no SA1 or SA3) | Unlabeled SA1 or SA3
Probe | Brain tissue* | Control (no SA1 or SA3) | 0.01 mg/kg | 0.1 mg/kg | 1.0 mg/kg
Probe | Brain tissue* | % Injected dose/g tissue
[ ^ 11 ^ C]SA1 | Cerebellum | 1.98 ± 0.20 | 1.95 ± 0.33 | 1.76 ± 0.12 | 1.45 ± 0.30**
[ ^ 11 ^ C]SA1 | Medulla oblongata | 2.29 ± 0.30 | 2.38 ± 0.40 | 2.00 ± 0.23 | 1.72 ± 0.40**
[ ^ 11 ^ C]SA3 | Cerebellum | 1.72 ± 0.17 | 1.72 ± 0.26 | 1.62 ± 0.36 | 1.43 ± 0.21
[ ^ 11 ^ C]SA3 | Medulla oblongata | 2.18 ± 0.19 | 2.22 ± 0.36 | 2.27 ± 0.49 | 1.87 ± 0.34

* For uptake in other tissues of the brain, see Toyohara et al. ( 1 ). ** P < 0.05.

In another study, it was shown that pretreatment of the mice (n = 5 animals) with ALX-5407 (10 mg/kg body weight), a sarcosine-based irreversible inhibitor of GlyT-1, decreased the accumulation of radioactivity from [^11^C]SA1 significantly (P < 0.05) in the cerebellum and the medulla oblongata of the animals compared to controls (1). No significant reduction in uptake of label in these brain tissues was noticed when the animals were pretreated with SSR504734, a non-sarcosine–based competitive inhibitor of GlyT-1. From these observations, the investigators concluded that endogenous concentrations of Gly in the mouse brain competed with SSR504734 and affected its binding to GlyT-1 in the tissues.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DSA1%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DSA1%20Non-Human%20Primates&cmd=DetailsSearch)]

Seven rhesus monkeys were used for PET imaging studies with [^11^C]SA1 as described by Toyohara et al. (1). The animals were injected with 1,180–1,380 MBq/7.8–77.9 nmol (31.86–37.26 mCi/7.8–77.9 nmol) [^11^C]SA1, and baseline PET images were acquired from conscious monkeys over the next 91 min. Another set of images were acquired for the same duration after blocking with ALX-5407 (3 mg/kg body weight) or SSR504734 (3 mg/kg body weight) as described elsewhere (1). Magnetic resonance images were used to define the regions of interest (ROI) for the frontal cortex, thalamus, brain stem, and cerebellum on the PET images to calculate the standard uptake values (SUV) for each ROI. In addition, the total volume of distribution (V_T_) of [^11^C]SA1 for the brain tissues was evaluated as described elsewhere (1). From the baseline scans it was evident that the label peaked in the four regions of the brain between 10 min and 30 min p.i. and decreased slightly thereafter, indicating that the label exhibited reversible kinetics.

Table 3: Standardized uptake values (SUV) and total volume of distribution (V _ T _ ) of [ ^ 11 ^ C]SA1 at baseline and in rhesus monkeys brain tissue pretreated with ALX-5407 and SSR504734. Data obtained from Toyohara et al. ( 1 ).

Brain tissue | Standardized uptake value (SUV) | | | Total volume of distribution (V _ T _ )
Brain tissue | Baseline* | Pretreated (3 mg/kg) | | Baseline | Pretreated (3 mg/kg)
Brain tissue | Baseline* | ALX-5407 | SSR504734 | Baseline | ALX-5407 | SSR504734
Brainstem | 1.5 ± 0.4 | 1.4 ± 0.2 | 1.3 ± 0.4 | 5.0 ± 2.3 | 4.3 ± 1.4 | 4.5 ± 2.1
Thalamus | 1.7 ± 0.5 | 1.6 ± 0.1 | 1.6 ± 0.5 | 5.6 ± 2.6 | 5.0 ± 1.4 | 5.5 ± 2.6
Frontal cortex | 1.3 ± 0.3 | 1.4 ± 0.1 | 1.3 ± 0.4 | 4.5 ± 2.0 | 4.5 ± 1.2 | 4.6 ± 2.1
Cerebellum | 1.4 ± 0.3 | 1.3 ± 0.1 | 1.3 ± 0.3 | 4.5 ± 2.0 | 4.2 ± 1.0 | 4.4 ± 2.0

*For the baseline group, n = 7 animals; for the pretreated group, n = 4 monkeys/GlyT-1 inhibitor.

The baseline SUVs toward the end of the scans were thalamus ≈ brain stem > cerebellum ≈ frontal cortex (Table 3). The baseline parametric V_T_ images showed that the distribution of [^11^C]SA1 in the brain was thalamus > brain stem > cerebellum ≈ frontal cortex (Table 3). All four regions of the brain from monkeys pretreated with ALX-5407 or SSR504734 showed little change in SUV or V_T_ of [^11^C]SA1 compared to the baseline values (1). The investigators mentioned that the nearly complete lack of change in the SUV or the V_T_ values was probably because the dose of GlyT-1 inhibitors used in the monkey study (3 mg/kg body weight) was insufficient to block the transporter. For ethical reasons, higher doses of the inhibitors were not administered to the animals due to the possibility of inducing pharmacological side effects in the monkeys.

The investigators concluded that among the three ^11^C-labeled GlyT-1 inhibitors evaluated in mice and non-human primates, only [^11^C]SA1 showed a suitable imaging profile and could be used only in rodents (1). Blocking studies with this tracer in conscious monkeys showed that it was unsuitable to visualize GlyT-1 in the brain of non-human primates. Therefore, the chemical structure of [^11^C]SA1 will have to be modified appropriately in order to use it as an in vivo imaging agent for the visualization of GlyT-1 in monkeys and humans (1).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B11C%5DSA1%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Toyohara J., Ishiwata K., Sakata M., Wu J., Nishiyama S., Tsukada H., Hashimoto K. (2011). In vivo evaluation of carbon-11-labelled non-sarcosine-based glycine transporter 1 inhibitors in mice and conscious monkeys. Nucl Med Biol.
2 Paoletti P. (2011). Molecular basis of NMDA receptor functional diversity. Eur J Neurosci.
3 Shim S.S., Hammonds M.D., Kee B.S. (2008). Potentiation of the NMDA receptor in the treatment of schizophrenia: focused on the glycine site. Eur Arch Psychiatry Clin Neurosci.
4 Hashimoto K. (2011). Glycine transporter-1: a new potential therapeutic target for schizophrenia. Curr Pharm Des.
5 Wolkenberg S.E., Sur C. (2010). Recent progress in the discovery of non-sarcosine based GlyT1 inhibitors. Curr Top Med Chem.
6 Hamill T.G., Eng W., Jennings A., Lewis R., Thomas S., Wood S., Street L., Wisnoski D., Wolkenberg S., Lindsley C., Sanabria-Bohorquez S.M., Patel S., Riffel K., Ryan C., Cook J., Sur C., Burns H.D., Hargreaves R. (2011). The synthesis and preclinical evaluation in rhesus monkey of [(1)F]MK-6577 and [(1)(1)C]CMPyPB glycine transporter 1 positron emission tomography radiotracers. Synapse.
7 Gunn R.N., Murthy V., Catafau A.M., Searle G., Bullich S., Slifstein M., Ouellet D., Zamuner S., Herance R., Salinas C., Pardo-Lozano R., Rabiner E.A., Farre M., Laruelle M. (2011). Translational characterization of [(11) C]GSK931145, a PET ligand for the glycine transporter type 1. Synapse.